# Lactoferrin-conjugated superparamagnetic iron oxide nanoparticles

Chemical name: | Lactoferrin-conjugated superparamagnetic iron oxide nanoparticles
Abbreviated name: | Lf-SPIONs
Synonym:
Agent Category: | Nanoparticles
Target: | Lactoferrin receptors
Target Category: | Receptors
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=BBB%20and%20review%20and%20delivery)]

The lactoferrin (Lf)-conjugated superparamagnetic iron oxide nanoparticles (SPIONs), abbreviated as Lf-SPIONs, was synthesized by Xie et al. for use as a contrast agent for magnetic resonance imaging (MRI) of brain tumors (1).

The blood–brain barrier (BBB) is composed of tight junction-sealed brain capillary endothelial cells (BCECs) and supporting pericytes and astrocytic endfeet (2). Exogenous compounds are prevented by the BBB from reaching the brain by passive transport or through the paracellular route (3). Because many proteins including Lf could effectively cross the BBB through transcytosis, an active transport mechanism of BCECs, this mechanism has been actively used to design brain-targeted delivery systems for targeted imaging and therapy of neurological diseases (4, 5).

Mammalian Lf is a cationic iron-binding glycoprotein (80 kDa), and its receptor expresses on the endothelial cells of the BBB (6). Upon binding with its receptor, Lf could cross the BBB through receptor-mediated transcytosis (5). The transport of Lf across the BBB is unidirectional, from the apical side to the basolateral side, with no apparent intraendothelial degradation (7, 8). Studies with membrane preparations of mouse brain have shown that the Lf receptor in the BCECs has two classes of binding sites: a high-affinity site that has a dissociation constant (K_d_) of 10.61 nM and a B_max_ of 410 fmol bound/µg protein; and a low-affinity site that has a K_d_ of 2,228 nM and a B_max_ of 51,641 fmol bound/µg protein (5). The plasma concentration of endogenous Lf (~5 nM) is lower than the K_d_ of Lf receptors in the BBB, which avoids the competitive inhibition of endogenous Lf to exogenous Lf-conjugated agents (8). The Lf receptor has also been shown to be overexpressed in various tumors, including brain glioma (1). Because of these features, Lf has been applied as a ligand in designing brain-targeted delivery systems.

Xie et al. developed the contrast agent Lf-SPIONs by conjugating Lf to SPIONs (1), while Qiao et al. developed the agent Fe_3_O_4_-Lf by conjugating Lf to Fe_3_O_4_ nanoparticles through polyethylene glycol (8). For the former agent, Lf was designed to target Lf-SPIONs to Lf receptor-expressing tumors. For the latter agent, Lf served to enhance the BBB-penetrating ability of Fe_3_O_4_-Lf by targeting Lf receptors expressed in the BCECs. Studies with the two agents showed that Lf-SPIONs were able to effectively enhance the glioma contrast, and that Fe_3_O_4_-Lf could effectively penetrate the BBB in healthy rats because of the conjugation of Lf (1, 8). This chapter summarizes the data obtained by Xie et al. with Lf-SPIONs (1).

### Related Resource Links:

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=lactoferrin) and protein (http://www.ncbi.nlm.nih.gov/protein?term=lactoferrin) of lactoferrin

Protein (http://www.ncbi.nlm.nih.gov/protein?term=lactoferrin%20receptor) of lactoferrin receptor

Lactoferrin-related clinical trials (http://clinicaltrials.gov/ct2/results?term=lactoferrin&Search=Search) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20970851)]

Xie et al. first modified SPIONs with meso-2,3-dimercaptosuccinic acid and then conjugated to Lf through classic EDC/sulfo-NHS-mediated amidation reaction (1). The final products, Lf-SPIONs, were collected with magnetic separation and dispersed in phosphate-buffered saline. The chemical yield and purity of Fe_3_O_4_-Lf were not reported.

Lf conjugation was evaluated with polyacrylamide gel electrophoresis and Fourier transform infrared spectroscopy (FTIR). Gel electrophoresis showed the specific band of Lf-SPIONs. FTIR showed the characteristic spectra of Lf-SPIONs, presenting peaks at ~1,668 cm−^1^ for the amide I band and at ~1,562 cm−^1^ for the amide II band. Peaks from bare SPIONs were observed at ~630, 590, and 450 cm−^1^, typical for Fe–O absorption bands. Lf was estimated to be 0.1 mg/mg SPIONs with the Bradford method. Bare SPIONs and Lf-SPIONs showed similar morphology under transmission electron microscopy (TEM). The size increased from 9.2 ± 0.4 nm for bare SPIONs to 13.6 ± 0.7 nm for Lf-SPIONs. The Lf-SPIONs dispersed in water had a hydrodynamic diameter of 74.8 ± 11.5 nm, larger than the hydrodynamic diameter of the SPIONs (62.0 ± 12.1 nm). The number of Lf per SPION was not reported.

The magnetic properties of SPIONs and Lf-SPIONs at room temperature were measured with vibrating sample magnetometry, exhibiting the saturation magnetization of 51 emu/g Fe for the Lf-SPIONs, lower than 78 emu/g Fe for the bare SPIONs, suggesting that Lf conjugation slightly changed the physical properties of SPIONs. MRI studies on the agent-mixing agarose gel phantoms showed that Lf-SPIONs could reduce the transverse relaxation time T2. With the increase of Lf-SPIONs concentration in the phantom, the signal intensity decreased and the relaxation curves became steeper. The R2 relaxivity coefficient values for Lf-SPIONs and SPIONs were 75.6 mM^–1^s^–1^ and 131.4 mM^–1^s^–1^, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20970851)]

Three cell lines including human embryonic kidney 293 (HEK 293), human normal liver cell line (HL-7702), and human umbilical vein endothelial cell line (ECV 304) were used to test the cell viability after exposure to bare SPIONs or Lf-SPIONs at concentrations of 0, 25, 50, 75, and 100 μg/mL Fe, respectively (1). Both SPIONs and Lf-SPIONs within the concentration range didn’t affect the cell viability as demonstrated with MTT (3-(4,5-dimethylthiazol-2-yl)-2,5-diphenyltetrazolium bromide) assays.

Internalization of the particles was measured with fast sequential atomic absorption spectrometry (AAS) and observed under TEM after incubation of C6 glioma cells with SPIONs and Lf-SPIONs at different iron concentrations (5, 10, 15, and 20 μg/mL) at 37°C for 0.5 h. The cellular uptake of Lf-SPIONs presented a dose-dependent, increasing adsorption curve on AAS. Lf-SPIONs accumulated in the cytoplasm of C6 cells on TEM images.

On MRI images (3.0 T) of the cell-embedded agarose phantoms, the signal intensity of C6 glioma cells treated with Lf-SPIONs at 1 μg/mL decreased markedly, whereas only negligible MRI contrast was observed from the control cells and the cells treated with bare SPIONs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20970851)]

In vivo MRI studies of Lf-SPIONs were performed with male, brain glioma-bearing Wistar rats (n = 9) after injection with SPIONs or Lf-SPIONs (12 mg Fe/kg) (1). High contrast of the brain glioma was observed with Lf-SPIONs between 2 h and 48 h after injection, but MRI with SPIONs showed no visible change over the same period. The decrease of MRI signal intensity in tumors was 36%–74% with Lf-SPIONs, as compared with the pre-contrasted tumors. Histology and Prussian staining of the tumor samples confirmed the presence of significant amount of Lf-SPIONs around vascular region of the tumor tissue at 48 h after injection. At high magnification (500×), Lf-SPIONs were observed to be within the cells. Poor in vivo uptake of SPIONs by the glioma cells was also verified with the same methods.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Xie H., Zhu Y., Jiang W., Zhou Q., Yang H., Gu N., Zhang Y., Xu H., Yang X. (2011). Lactoferrin-conjugated superparamagnetic iron oxide nanoparticles as a specific MRI contrast agent for detection of brain glioma in vivo. Biomaterials.
2 Fortin D. (2012). The blood-brain barrier: its influence in the treatment of brain tumors metastases. Curr Cancer Drug Targets.
3 Fu B.M. (2012). Experimental methods and transport models for drug delivery across the blood-brain barrier. Curr Pharm Biotechnol.
4 Huang R., Ke W., Han L., Liu Y., Shao K., Jiang C., Pei Y. (2010). Lactoferrin-modified nanoparticles could mediate efficient gene delivery to the brain in vivo. Brain Res Bull.
5 Huang R.Q., Ke W.L., Qu Y.H., Zhu J.H., Pei Y.Y., Jiang C. (2007). Characterization of lactoferrin receptor in brain endothelial capillary cells and mouse brain. J Biomed Sci.
6 Suzuki Y.A., Lopez V., Lonnerdal B. (2005). Mammalian lactoferrin receptors: structure and function. Cell Mol Life Sci.
7 Fillebeen C., Descamps L., Dehouck M.P., Fenart L., Benaissa M., Spik G., Cecchelli R., Pierce A. (1999). Receptor-mediated transcytosis of lactoferrin through the blood-brain barrier. J Biol Chem.
8 Qiao R., Jia Q., Huwel S., Xia R., Liu T., Gao F., Galla H.J., Gao M. (2012). Receptor-mediated delivery of magnetic nanoparticles across the blood-brain barrier. ACS Nano.